# ^111^In-DOTA-4-amino-1-carboxymethyl-piperidine-D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_

Chemical name: | ^111^In-DOTA-4-amino-1-carboxymethyl-piperidine-D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_
Abbreviated name: | ^111^In-RM2
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal\contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20RM2)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptor (GRPR) with high affinity and specificity (1). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system (CNS) and the gastrointestinal (GI) system. They also act as potential growth factors for both normal and neoplastic tissues (2). Specific BBN receptors have been identified on CNS and GI tissues, including the pancreas, and on a number of tumor cell lines. The BBN-receptor superfamily includes at least four different subtypes, namely neuromedin B (NMB or BB1), the GRPR subtype (BB2), the BB3 subtype, and the BB4 subtype (3). The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR.

Currently used targeting GRPR peptides are primarily agonists. Therefore, there is a need for GRPR antagonist radioligands. Llinares et al. (4) developed a series of GRPR peptide antagonists. One of them, D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_ (RM26), has been found to be a selective GRPR antagonist. A DOTA-Gly-benzoyl group was added to the C-terminus to form DOTA-Gly-benzoyl-D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_ (RM1). For evaluation as a single-photon emission computed tomography (SPECT) imaging agent for GRPR, ^111^In has been attached to RM1 to form ^111^In-RM1 (http://www.ncbi.nlm.nih.gov/books/NBK23333/) (5). A new GRPR peptide antagonist, DOTA-4-amino-1-carboxymethyl-piperidine-D-Phe-Gln-Trp-Ala-Val-Gly-His-Sta-Leu-NH_2_ (RM2), has been found to have a higher affinity for GRPR than RM1 and has been labeled with ^111^In for single-photon emission computed tomography (SPECT) imaging (6).

### Related Resource Links:

- Chapters in MICAD (GRPR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=GRPR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (GRPR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925)).
- Articles in OMIM (GRPR (http://www.ncbi.nlm.nih.gov/omim/305670))
- Clinical trials (GRPR (http://www.clinicaltrials.gov/ct2/results?term=Gastrin-releasing+peptide+receptor+))
- Drug information in FDA (GRPR (http://google-test.fda.gov/search?q=GASTRIN-RELEASING+PEPTIDE+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20RM2+synthesis)]

RM2 was prepared by solid-phase peptide synthesis with >70% yield (6). ^111^InCl_3_ was added to a solution of RM2 (~6 nmol) in sodium acetate (pH 5). The mixture was heated for 30 min at 95°C. The product, ^111^In-RM2, was identified with electrospray-mass spectrometry and used without further purification. The labeling yield of ^111^In-RM2 was >95%, with a specific activity of 30 GBq/µmol (0.81 Ci/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20RM2+in+vitro)]

Mansi et al. (6) performed in vitro inhibition studies of RM1, ^nat^In-RM1, RM2, and ^nat^In-RM2 in cultured PC-3 human prostate cells with ^125^I-BBN; Mansi et al. recorded 50% inhibition concentration (IC_50_) values of 35.0 ± 13.0, 14.0 ± 3.4 nM, 7.7 ± 3.3, and 9.3 ± 3.3, respectively. ^111^In-RM1 showed a K_d_ value (affinity constant) of 8.5 ± 2.7 nM and a B_max_ value (receptor density) of 2.4 ± 0.2 nM, whereas ^111^In-RM2 showed a higher affinity (K_d_, 2.9 ± 0.4 nM) and a lower receptor density (B_max_, 1.1 ± 0.1 nM). PC-3 cells exhibited a 3.7% uptake of the ^111^In-RM2 incubation dose at 4 h of incubation at 37°C, with 15.9% of the incubation dose remaining on the cell surface, which indicated a lack of cell internalization of the radioligand. RM2 was able to inhibit the calcium release and receptor internalization induced by BBN indicating antagonist behavior.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20RM2+rodentia)]

Mansi et al. (6) performed ex vivo biodistribution studies of 0.18 MBq (5 μCi) ^111^In-RM2 in nude mice (n = 4/group) bearing PC-3 tumors. Tumor accumulation values for ^111^In-RM2 were 15.2 ± 4.8, 11.8 ± 2.4, and 6.8 ± 1.0% injected dose per gram (ID/g) at 1, 4, and 24 h after injection, respectively. ^111^In-RM2 exhibited a fast blood clearance, with 0.05% ID/g at 4 h after injection. The tumor/blood ratios were 20, 235, and 2,280 at 1, 4, and 24 h after injection, respectively. The initial accumulation was high in the pancreas, kidney, pituitary adrenal, stomach, and intestine at 1 h after injection, with rapid washout by 4 h. Preinjection of excess RM2 peptide (20 nmol, 5 min) inhibited the GRPR-positive tumor, pancreas, stomach, and intestine accumulation by ~90%, with little effect in the other tissues at 4 h after injection.

SPECT imaging in nude mice (n = 2) bearing PC-3 xenografts was performed with 42 MBq (1.1 mCi) ^111^In-RM2 at 24 after injection. The tumors, kidneys, and urinary bladder were clearly visualized. No blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20RM2+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20RM2+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In%20RM2+human)]

No publication is currently available.

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
3 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
4 Llinares M., Devin C., Chaloin O., Azay J., Noel-Artis A.M., Bernad N., Fehrentz J.A., Martinez J. (1999). Syntheses and biological activities of potent bombesin receptor antagonists. J Pept Res.
5 Mansi R., Wang X., Forrer F., Kneifel S., Tamma M.L., Waser B., Cescato R., Reubi J.C., Maecke H.R. (2009). Evaluation of a 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-conjugated bombesin-based radioantagonist for the labeling with single-photon emission computed tomography, positron emission tomography, and therapeutic radionuclides. Clin Cancer Res.
6 Mansi R., Wang X., Forrer F., Waser B., Cescato R., Graham K., Borkowski S., Reubi J.C., Maecke H.R. (2011). Development of a potent DOTA-conjugated bombesin antagonist for targeting GRPr-positive tumours. Eur J Nucl Med Mol Imaging.